# ^99m^Tc-Labeled N-(triethylammonium)-3-propyl-[15]ane-N5

Chemical name: | ^99m^Tc-Labeled N-(triethylammonium)-3-propyl-[15]ane-N5 | [image]
Abbreviated name: | [^99m^Tc]NTP 15-5 | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Cartilage proteoglycans | [image]
Target Category: | Others (heavily glycosylated glycoproteins) | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Given above is the structure of [^99m^Tc]NTP 15-5 (1). Click here (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=glyco2&part=ch16) for information regarding proteoglycans and sulfated glycosaaminoglycans (2).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cartilage+proteoglycans)]

Chondrosarcomas are the second most common primary malignancies of the skeleton. These cancers have a characteristic slow growth and overproduce extracellular matrix (ECM) of the cartilage. The ECM of the cartilage is composed of several components, including proteoglycans, which have been described in detail by Gentili and Cancedda (3). Proteoglycans are negatively charged molecules, impart elasticity to the structure (3), and have been targeted with quaternary ammonium compounds (QAC), which carry a high positive charge, for the selective delivery of drugs or radioactive isotopes to the cartilage (1). Because of their specificity of binding of QACs to the cartilage, the QAC ^99m^Tc-labeled N-(triethylammonium)-3-propyl-[15]ane-N5 ([^99m^Tc]NTP 15-5) was synthesized (4) and studied for its pharmacokinetic behavior and biodistribution in rats (5). [^99m^Tc]NTP 15-5 has also been evaluated for the imaging of cartilage integrity and osteoarthritis in rabbits (6) and guinea pigs (1), respectively. More recently, [^99m^Tc]NTP 15-5 was used for the detection of grade II chondrosarcoma in a rat model (7).

### Other sources of information

Cartilage proteoglycans in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=cartilage%20proteoglycans).

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Cartilage+proteoglycans) on cartilage proteoglycans.

Drug and other information regarding proteoglycan inhibitors – FDA (http://google2.fda.gov/search?q=Proteoglycan+inhibitors&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=17&y=15).

Information on proteoglycan structure (http://www.ncbi.nlm.nih.gov/pubmed?term=Proteoglycan%20structure&cmd=DetailsSearch), function (http://www.ncbi.nlm.nih.gov/pubmed?term=Proteoglycan%20function&cmd=DetailsSearch) and role in cancer (http://www.ncbi.nlm.nih.gov/pubmed?term=proteoglycan%20and%20cancer&cmd=DetailsSearch) in PubMed.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NTP+15-5+synthesis)]

The synthesis of NTP 15-5 is described in detail elsewhere (4), and its labeling with ^99m^Tc was described by Ollier et al. (6). The radiochemical yield of the radiotracer was ~100% with a purity of >98% (6) as determined with thin-layer chromatography and high-pressure liquid chromatography, respectively (4). The specific activity of [^99m^Tc]NTP 15-5 was reported to be 23 MBq/μmol (0.86 mCi/μmol), and the tracer was stable at room temperature for >24 h at pH 7.0 (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+NTP+15-5+in+vitro)]

The binding of [^99m^Tc]NTP 15-5 to proteoglycans was investigated by incubating the radiochemical with cultured rabbit articular chondrocytes for 24 h (5). The culture medium was then dialyzed against increasing pH buffers (pH ranging from 5.0 to 11.0), and radioactivity bound to proteoglycans was separated for measurement with Sepharose 2B chromatography as described by Maurizis et al. (8). Only half of the radiolabeled compound that bound to the proteoglycans was reported to dissociate from the complexes at pH 8.5.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+NTP+15-5+rodentia)]

Maurizis et al. studied the biodistribution of [^99m^Tc]NTP 15-5 in Sprague-Dawley rats (n = 5) (5). The animals were euthanized at 10 min and 1 h after the radiochemical was administered through the tail vein. Select tissues were then taken from the animals to measure accumulated radioactivity and presented as a percent of injected dose per gram tissue (% ID/g). At 10 min after administration, maximum radioactivity was detected in the kidneys (6.02 ± 2.04% ID/g) followed by the articular cartilage (2.18 ± 0.41% ID/g), intervertebral disc (1.87 ± 0.35% ID/g), liver (1.22 ± 0.25% ID/g), and plasma (1.04 ± 0.17% ID/g). The other tissues (blood, bone, and muscle) had a label accumulation between 0.15 ± 0.05% ID/g (bone) and 0.63 ± 0.14% ID/g (blood). At 1 h, the accumulated tracer levels were 3.51 ± 0.47% ID/g (kidney), 2.04 ± 0.38% ID/g (liver), 1.29 ± 0.22% ID/g (articular cartilage), and 0.68 ± 0.14% ID/g (intervertebular cartilage). The other organs had <0.1% ID/g accumulated radioactivity at this time point. This study showed that [^99m^Tc]NTP 15-5 was eliminated from the system primarily through the urinary route and, unlike other tissues, accumulated mainly in the cartilages. No blocking studies were reported.

In another study using a primary model (paratibial location; n = 12 animals) and a recurrence model (located on the femoral condyle; n = 9 animals), Miot-Noirault et al. evaluated the application of [^99m^Tc]NTP 15-5 scintigraphy for the detection of Swarm chondrosarcomas in rats (7). Scintigraphy was performed on the treated animals at predetermined intervals for 50 days, and results obtained with [^99m^Tc]NTP 15-5 were compared with those obtained with [^99m^Tc]-hydroxymethylenediphosphonate ([^99m^Tc]-HMDP) scanning during the same period. Although repeat injections of [^99m^Tc]NTP 15-5 and ^99m^Tc-HMDP were reported to be well tolerated by the animals it was not clear if the rats were injected repeatedly by the investigators to study the use of these tracers for tumor scintigraphy over a period of 50 days. With [^99m^Tc]NTP 15-5, the mean target/background ratio for the primary model increased from 1.6 ± 0.14 at day 4 to 4.25 ± 0.25 on day 45, and for the recurrence model it increased from 3.27 ± 0.24 at day 4 to 5.25 ± 0.49 on day 50. However, during the entire period of the study, all ^99m^Tc-HMDP scans were negative. From these results the investigators concluded that [^99m^Tc]NTP 15-5 could be used for the imaging of primary and recurrent chondrosarcoma growth in rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Ollier et al. compared the use of [^99m^Tc]NTP 15-5 and [^99m^Tc]methylenediphosphonate ([^99m^Tc]MDP) to detect papain-induced arthrosis (n = 6 animals/group), zymosan-induced arthritis (n = 5 animals/group), and the effect of aging (n = 5 animals/group) on rabbit knee bone joints with scintigraphic imaging with the radiochemicals for up to 60 days after the induction of arthrosis and arthritis (6). Imaging was performed between 5 min and 2 h after an injection of [^99m^Tc]NTP 15-5 and after between 1 and 3 h for animals given [^99m^Tc]MDP. From these studies the investigators concluded that, although both imaging agents were quite similar in detecting cartilage degradation due to arthrosis, arthritis, or aging of the rabbit knee joint, images obtained with [^99m^Tc]NTP 15-5 were superior to those obtained with [^99m^Tc]MDP, probably because NTP accumulates in the cartilage while MDP accumulation correlates more with metabolic activity of the osteoblasts and depends on the level of hydroxyapatite in the skeletal tissue.

In another study, the scintigraphic use of [^99m^Tc]NTP 15-5 and [^99m^Tc]MDP was evaluated to detect osteoarthritis in guinea pigs after a medial meniscectomy (MNX; n = 10 animals), which is the removal of the medial meniscus, a “C-shaped” cartilage that is attached to the tibial head of the knee joint and acts as a shock-absorbing material for the knee, or a sham operation (n = 5 animals) (1). Imaging was performed on the joints at predetermined time points from 20 to 180 days after the surgery, and data were presented as scintigraphic ratios of the operated/contralateral femoral (F) and tibial (T) areas (FTR) for both imaging agents. Imaging on the animals was performed at the various time points 15 min after an injection of the respective tracers. With [^99m^Tc]NTP 15-5, the FTR values in animals after MNX were higher (F = 1.7 ± 0.2 and T = 1.6 ± 0.1) than those for animals with sham operations (F = 1.0 ± 0.1 and T = 1.0 ± 0.1) 50 days after the surgery. However, at 180 days after surgery the FTR values were significantly lower in the MNX animals (F = 0.6 ± 0.1 and T = 0.7 ± 0.1) than in animals with the sham operation (F = 1.0 ± 0.1 and T = 0.9 ± 0.1). With [^99m^Tc]MDP, no change in FTR values was noticed during the 180 days. A microscopic examination of the MNX joints confirmed the presence of osteoarthritis, and no such change was observed in the joints of animals with the sham surgery. From this study the investigators concluded that [^99m^Tc]NTP 15-5 was suitable for imaging osteoarthritis under in vivo conditions.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+NTP+15-5+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+NTP+15-5+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## References

1 Miot-Noirault E., Vidal A., Pastoureau P., Bonafous J., Chomel A., Sarry L., Audin L., Madelmont J.C., Moins N. (2007). Early detection and monitoring of cartilage alteration in the experimental meniscectomised guinea pig model of osteoarthritis by 99mTc-NTP 15-5 scintigraphy. Eur J Nucl Med Mol Imaging.
2 Esko, J.D., K. Kimata, and U. Lindhal, Proteoglycans and Sulfated Glycosaaminoglycans. 2nd ed. Essentials of Glycobiology, ed. A. Varki, R.D. Cummings, J.D. Esko, H.H. Freeze, P. Stanley, C.R. Bertozzi, G.W. Hart, and M.E. Etzler. 2009, Plainview (NY): Cold Spring Harbor Laboratory Press. 784 pp.
3 Gentili C., Cancedda R. (2009). Cartilage and bone extracellular matrix. Curr Pharm Des.
4 Nicolas C., Borel M., Maurizis J.C., Gallais N., Rapp M., Ollier M., Verny M., Madelmont J.C. (2000). Synthesis of N-quaternary ammonium 3H and 99mTc-polyazamacrocycles, potential radiotracers for cartilage imaging. J. Labelled Cpd. Radiopharm.
5 Maurizis J.C., Rapp M., Nicolas C., Ollier M., Verny M., Madelmont J.C. (2000). Disposition in rats of N-pyridinium-propyl-cyclam, N-triethylammonium-propyl-cyclam, and N-[Triethylammonium]-3-propyl-[15]ane-N5, potential cartilage imaging agents. Drug Metab Dispos.
6 Ollier M., Maurizis J.C., Nicolas C., Bonafous J., de Latour M., Veyre A., Madelmont J.C. (2001). Joint scintigraphy in rabbits with 99mtc-N-[3-(triethylammonio)propyl]-15ane-N5, a new radiodiagnostic agent for articular cartilage imaging. J Nucl Med.
7 Miot-Noirault E., Gouin F., Vidal A., Rapp M., Maublant J., Askienazy S., Chezal J.M., Heymann D., Redini F., Moins N. (2009). First Preclinical Imaging of Primary Cartilage Neoplasm and Its Local Recurrence Using 99mTc-NTP 15-5 Radiotracer. J Nucl Med.
8 Maurizis J.C., Ollier M., Nicolas C., Madelmont J.C., Garrigue H., Veyre A. (1992). In vitro binding of oxime acetylcholinesterase reactivators to proteoglycans synthesized by cultured chondrocytes and fibroblasts. Biochem Pharmacol.